# N-Acetyl-N-(2-[^11^C]methoxybenzyl)-2-phenoxy-5-pyridinamine

Chemical name: | N-Acetyl-N-(2-[^11^C]methoxybenzyl)-2-phenoxy-5-pyridinamine
Abbreviated name: | [^11^C]PBR28
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Human Primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR28%5BAll%20Fields%5D)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as central benzodiazepine receptors (CBR) and peripheral benzodiazepine receptors (PBR, also known as translocator protein (TSPO)). The CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4).The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo by positron emission tomography (8) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity. [^11^C]PK11195 has been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the central nervous system (9, 10). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than PK11195 (9, 10). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET ligands with highly selective and specific binding to PBR. N-Acetyl-N-(2-methoxybenzyl)-2-phenoxy-5-pyridinamine (PBR28), which has an aryloxyanilide structure, has been shown to have high affinity and selectivity for PBR (11). N-Acetyl-N-(2-[^11^C]methoxybenzyl)-2-phenoxy-5-pyridinamine ([^11^C]PBR28) has been developed for imaging PBR in the brain.

### Related Resource Links:

- Chapters in MICAD (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (PBR (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610))
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))
- Drug information in FDA (PBR (http://google2.fda.gov/search?q=Peripheral-type+benzodiazepine+receptor+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=5&y=5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR28%20and%20synthesis)]

Imaizumi et al. (11) reported the synthesis of [^11^C]PBR28 by ^11^C-methylation of the O-desmethyl precursor with [^11^C]CH_3_I. [^11^C]PBR28 was purified by high-performance liquid chromatography (HPLC). The specific activity was 59.7 ± 2.7 GBq/μmol (1.61 ± 0.07 Ci/μmol) at the time of injection. Time of synthesis or radiochemical yield was not reported. Wang et al. (12) reported a fully automated synthesis of [^11^C]PBR28 using [^11^C]methyl triflate and the O-desmethyl precursor with radiochemical yields (decay-corrected) of 70-80% based on [^11^C]CO_2_ at the end of bombardment (EOB). The overall synthesis, HPLC purification and formulation time was 25-30 min from EOB. The specific radioactivity was in a range of 185-555 GBq/μmol (5-15 Ci/μmol) at EOB with >99% radiochemical purity.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR28%20and%20in%20vitro)]

In vitro [^3^H]PK11195 PBR-binding studies showed that PBR28 had an IC_50_ value of 0.6 nM. PBR28 has a lipophilicity value of 2.98 and little activity against various neurotransmitters and transporters (11). PBR28 showed inhibition constant (K_i_) values >10 µM for several CBR subtypes.

Owen et al. (13) performed in vitro binding studies using human post-mortem brain tissues from normal subjects without any history of neurologic disease with [^3^H]PBR28. PBR28 binds to PBR with high affinity (K_i_ = 3.4 ± 0.2 nM, n = 6 (40%), low affinity (K_i_ = 188 ± 7 nM, n = 5 (33%)), and mixed affinity (two sites: K_i_ = 4.0 ± 1.2 nM (high), K_i_ = 313 ± 38 nM (low), n = 4 (27%)). Differences in affinity between high affinity binders (HABs) and low affinity binders (LABs) are ~55-fold with PBR28, ~17-fold with PBR06, and ~4-fold with DA1106, DPA713 and PBR111. Mixed affinity binders (MABs) express one class of sites with an affinity, which approximately equal to the means of those for HABs and LABs. PBR28 is a more dominant mixed affinity ligand than PBR06. PK11195 binds equally well to all with one affinity (K_i_ = ~23 nM, n =15 (100%)). In an autoradiography study with brain tissues from 22 donors, Owen et al. (14) showed 23% of samples (LABs) with no detectable specific signal with [^3^H]PBR28. The other samples showing signal were HABs (46%) and MABs (31%). On the other hand, all samples showed signal with [^3^H]PK11195. There was no difference in binding affinity or binding site density for [^3^H]PK11195 in samples showing no [^3^H]PBR28 signal.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR28%20and%20rodentia)]

Imaizumi et al. (11) reported PET studies of [^11^C]PBR28 to localize PBRs in a permanent middle cerebral artery occlusion model of neuroinflammation in the rat. Regional volume of distribution (V’_T_) was obtained by a two-compartment model with arterial input. In two bolus studies with scans up to 120 min, [^11^C]PBR28 was injected intravenously over 6 min. [^11^C]PBR28 showed high peak uptake of ~140, 170, and 200% standard uptake value in the contralateral side, the ischemic core, and the peri-ischemic core at 5–10 min after injection, respectively. Bolus to infusion (B/I) experiments were acquired with two different ratios (B/I = 2 and 5 h). There were 100–190% and 140–290% increases of V’_T_ in the ischemic core and the peri-ischemic core over the contralateral side, respectively. Injection of PK11195 (60 min after [^11^C]PBR28) reduced radioactivity in the ischemic core and the peri-ischemic core region to that of the contralateral region. In vitro autoradiographic studies of [^3^H]PK11195 showed significant correlation with the V’_T_ values of [^11^C]PBR28 PET obtained in the contralateral side, the ischemic core, and the peri-ischemic core. The increase of [^11^C]PBR28 binding in ischemic and peri-ischemic areas may represent a microglial activation because of cerebral artery occlusion.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR28%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR28%20and%20%28primate%20not%20human%29)]

Imaizumi et al. (15) performed brain (n = 6) and whole-body (n = 3) PET imaging in nonhuman primates after intravenous injection of [^11^C]PBR28. Brain accumulation of radioactivity peaked at ~40 min with 300% standardized uptake value (SUV). The gray matter had higher radioactivity than the white matter with the highest radioactivity in the choroid plexus of the 4^th^ ventricle. Co-injection of DAA1106 (3 mg/kg) reduced the SUV in the putamen to <100% at 80 min after injection. Whole-body PET scans showed that the BPR-positive organs such as lungs (56% injected dose (ID)), kidneys 7% ID), brain (6% ID) and heart (5% ID) exhibited moderate to high activity at 2-10 min after injection. Co-injection of PK 11195 (10 mg/kg) reduced the radioactivity in these organs by 50-70% at 60 min after injection.

## Human Studies

[Pub Med (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=PBR28%20and%20human)]

Fujita et al. (16) performed [^11^C]PBR28 PET brain scans in 12 healthy subjects for 120-180 min with one- and two-tissue compartmental analyses combined with serial radioactivity in arterial plasma. To obtain stable distribution volume (V_T_) values 90 min of imaging and two-tissue model were required. The V_T_ values in humans were only ~5% of those in monkeys. Two subjects (14%) showed no significant binding in the brain, and organs with the highest PBR densities such as the lungs and kidneys. Owen et al. (13) reported that the V_T_ values of three out of 35 (9%) healthy subjects could not be calculated because of low specific signal. It was concluded that these subjects are likely be to be LABs.

Brown et al. (17) performed dynamic whole-body scans after injection of 651 ± 111 MBq of [^11^C]PBR28 in seven healthy subjects for radiation dosimetry measurement. For six subjects, the three organs with the highest radioactivity were the kidneys, spleen and lungs (organs with the highest PBR densities). The effective dose was 6.6 ± 1.7 µSv/MBq. One subject showed 60-90% less radioactivity in these three organs, resulting in 28% lower effective dose.

## Supplemental Information

[Disclaimers (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=disclaimer)]

Synthesis Protocol

Toxicology

Preclinical Pharmacology

Clinical Pharmacology

## NIH Support

Intramural Research Program

## References

1 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
2 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Petit-Taboue M.C., Baron J.C., Barre L., Travere J.M., Speckel D., Camsonne R., MacKenzie E.T. (1991). Brain kinetics and specific binding of [11C]PK 11195 to omega 3 sites in baboons: positron emission tomography study. Eur J Pharmacol.
9 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
10 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
11 Imaizumi M., Kim H.J., Zoghbi S.S., Briard E., Hong J., Musachio J.L., Ruetzler C., Chuang D.M., Pike V.W., Innis R.B., Fujita M. (2007). PET imaging with [11C]PBR28 can localize and quantify upregulated peripheral benzodiazepine receptors associated with cerebral ischemia in rat. Neurosci Lett.
12 Wang M., Yoder K.K., Gao M., Mock B.H., Xu X.M., Saykin A.J., Hutchins G.D., Zheng Q.H. (2009). Fully automated synthesis and initial PET evaluation of [11C]PBR28. Bioorg Med Chem Lett.
13 Owen D.R., Gunn R.N., Rabiner E.A., Bennacef I., Fujita M., Kreisl W.C., Innis R.B., Pike V.W., Reynolds R., Matthews P.M., Parker C.A. (2011). Mixed-affinity binding in humans with 18-kDa translocator protein ligands. J Nucl Med.
14 Owen D.R., Howell O.W., Tang S.P., Wells L.A., Bennacef I., Bergstrom M., Gunn R.N., Rabiner E.A., Wilkins M.R., Reynolds R., Matthews P.M., Parker C.A. (2010). Two binding sites for [3H]PBR28 in human brain: implications for TSPO PET imaging of neuroinflammation. J Cereb Blood Flow Metab.
15 Imaizumi M., Briard E., Zoghbi S.S., Gourley J.P., Hong J., Fujimura Y., Pike V.W., Innis R.B., Fujita M. (2008). Brain and whole-body imaging in nonhuman primates of [11C]PBR28, a promising PET radioligand for peripheral benzodiazepine receptors. Neuroimage.
16 Fujita M., Imaizumi M., Zoghbi S.S., Fujimura Y., Farris A.G., Suhara T., Hong J., Pike V.W., Innis R.B. (2008). Kinetic analysis in healthy humans of a novel positron emission tomography radioligand to image the peripheral benzodiazepine receptor, a potential biomarker for inflammation. Neuroimage.
17 Brown A.K., Fujita M., Fujimura Y., Liow J.S., Stabin M., Ryu Y.H., Imaizumi M., Hong J., Pike V.W., Innis R.B. (2007). Radiation Dosimetry and Biodistribution in Monkey and Man of 11C-PBR28: A PET Radioligand to Image Inflammation. J Nucl Med.